# 4-[^18^F]Fluorobenzoyl-T84.66 diabody

Chemical name: | 4-[^18^F]Fluorobenzoyl-T84.66 diabody
Abbreviated name: | [^18^F]FB-T84.66 diabody
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-T84.66)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory states such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8). ^99m^Tc-Arcitumomab (a murine anti-CEA mAbFab’ fragment) was approved by the United States Food and Drug Administration in 1999 for whole-body planar and single-photon emission computed tomography (SPECT) imaging of CEA expression.

Single-chain variable fragments (scFvs) of antibodies with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) has been evaluated for targeting in several tumor antigen systems and has demonstrated rapid tumor localization and high-contrast imaging (9, 10). In particular, a murine anti-CEA T84.66 diabody, which retains excellent CEA-binding properties, was radiolabeled with ^124^I for localization of CEA-positive tumors in mice (11). However, for clinical development, ^18^F offers the advantages of easy availability, a higher positron yield (nearly 100% versus 23% for ^124^I), and a short half-life (109.7 min versus 4.18 days for ^124^I). Therefore, a diabody labeled with ^18^F is more suitable for routine clinical use because of the biological targeting and clearance kinetics of diabodies. 4-[^18^F]Fluorobenzoyl-T84.66 diabody ([^18^F]FB-T84.66 diabody) is being developed as a positron emission tomography (PET) agent to image CEA-expressing tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T84.66%20and%20synthesis)]

N-Succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) was synthesized in two steps from [^18^F]KF (Kryptofix 2.2.2./K_2_CO_3_) in 138 ± 8 min using a commercially available synthetic module with a radiochemical yield of 32.5 ± 5.9% (decay-corrected) (12). [^18^F]SFB was conjugated to T84.66 diabody to form [^18^F]FB-T84.66 diabody at 40°C for 30 min. [^18^F]FB-T84.66 diabody was isolated by gel filtration through PD-10 column with a radiochemical purity of >98%. The overall radiochemical yields were 1.40 ± 0.16% (decay-corrected). The specific activity was 1.83 ± 1.71 GBq/μmol (49.5 ± 46.2 Ci/μmol) at the end of synthesis. Total synthesis time was 35 ± 5 min starting from [^18^F]SFB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T84.66%20and%20in%20vitro)]

Radioimmunoreactivity of [^18^F]FB-T84.66 diabody for LS 174T human colon carcinoma cell (high CEA expression) was determined to be 57.1 ± 2.0% (n = 4) (12), higher than the previously reported value of 42% for the ^124^I-labeled T84.66 diabody (11). For CEA-negative C6 rat glioma cells, which are negative for CEA expression, [^18^F]FB-T84.66 diabody binding was 6.3 ± 1.6% (n = 4), indicating minimal nonspecific binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T84.66%20and%20rodentia)]

Cai et al. (12) performed biodistribution studies of [^18^F]FB-T84.66 diabody in nude mice (n = 4 mice/group) with the use of an LS174T subcutaneous xenograft model. Data were obtained at 1, 2, 4, and 6 h after injection. [^18^F]FB-T84.66 diabody had a rapid blood clearance, resulting in very low activity in the blood at 1 min and 2 h (2.08 ± 0.49% and 0.91 ± 0.21% injected dose (ID)/g, respectively). The initial tracer accumulation in the CEA-expressing tumor was 2.67 ± 1.05% ID/g at 1 h and decreased to ~1.8% ID/g at 2 h. At 1 h, the highest radioactivity was found in the liver, followed by the kidneys, spleen, and tumor. All other major organs exhibited background levels of radioactivity at all time points. The tracer had fast renal clearance. No defluorination of [^18^F]FB-T84.66 diabody was detected. The tumor/blood ratio increased significantly over time (1.31 ± 0.59, 2.20 ± 0.71, 3.24 ± 1.21, and 6.78 ± 2.26 at 1, 2, 4, and 6 h after injection, respectively; P < 0.05 in all cases). The tumor/muscle ratio also increased steadily over time (5.41 ± 2.30, 8.71 ± 5.72, 13.98 ± 8.29, and 29.52 ± 12.61 at 1, 2, 4, and 6 h after injection, respectively). No blocking experiment was performed.

[^18^F]FB-T84.66 diabody microPET imaging of mice bearing LS 174T or C6 tumors on the left front leg showed that the LS 174T tumors but not the C6 tumors were clearly visible at 30 min after injection (12). High uptake was observed in the liver, kidneys, and urinary bladder. LS 174T tumor uptake remained steady over time (2.55 ± 0.22, 2.37 ± 0.30, 2.22 ± 0.50, and 2.23 ± 0.17% ID/g at 0.5, 1, 2, and 4 h after injection, respectively). C6 tumor uptake was at the background level (0.90 ± 0.14, 0.71 ± 0.10, 0.53 ± 0.05, and 0.36 ± 0.15% ID/g at 0.5, 1, 2, and 4 h after injection, respectively) and was significantly lower than LS 174T tumor uptake at all time points examined (P < 0.05 in all cases).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T84.66%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T84.66%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T84.66%20and%20human)]

No publication is currently available.

## NIH Support

R21 EB001785, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862,

P01 CA43904, P50 CA86306, CA16042

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
12 Cai W., Olafsen T., Zhang X., Cao Q., Gambhir S.S., Williams L.E., Wu A.M., Chen X. (2007). PET Imaging of Colorectal Cancer in Xenograft-Bearing Mice by Use of an 18F-Labeled T84.66 Anti-Carcinoembryonic Antigen Diabody. J Nucl Med.